# Cross-linked iron oxide–transactivator transcription

Chemical name: | Cross-linked iron oxide– transactivator transcription
Abbreviated name: | CLIO-Tat
Synonym: | Cross-linked superparamagnetic iron oxide–Tat peptide, FITC-CLIO-Tat, CLIO-Tat(FITC), Tat-CLIO
Agent Category: | Iron oxide
Target: | Cell membrane
Target Category: | Adsorptive endocytosis, phagocytosis
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20AND%20tat)]

Investigation of cell migration could lead to understanding such biological events as embryogenesis development, functions of mature cells, vascular remodeling during angiogenesis, and most immune and infectious diseases. Because monitoring cell migration traditionally involves invasive methods such as intravital microscopy or flow cytometry analysis of cells recovered from excised tissue, it has been a long-sought goal to develop non-invasive imaging of cell migration in vivo. Because of recent advances in magnetic resonance imaging (MRI), magnetic labeling of cells is one of the techniques that can serve this purpose. Cells can be tagged with magnetic particles and then followed in vivo using MRI. Two of the common magnetic labeling techniques are: (A) attaching magnetic particles directly to the cell surface or (B) internalizing biocompatible magnetic particles by either endocytosis (fluid-phase or receptor-mediated) or phagocytosis. Surface attachment of magnetic particles can be efficient, but it is usually not applicable for in vivo purposes because of rapid reticuloendothelial clearance of these cells. On the other hand, lymphocytes and other cells have been used to internalize nanoparticles through fluid-phase or receptor-mediated endocytosis. However, these methods are generally not very efficient. It is therefore highly desirable to develop more efficient methods for intracellular magnetic labeling.

There are several peptides and proteins with membrane translocation properties that have been described, including penetrin (the third helix homeodomain of Antennapedia) (1), VP22 herpes virus protein (2, 3), anti-DNA monoclonal antibody and a derived peptide (4), and human immunodeficiency virus-1 transactivator transcription (HIV-1 Tat) protein (5). It is hypothesized that using one of the membrane translocation peptides would enable more efficient internalization of the magnetic nanoparticles into cells.

Superparamagnetic iron oxide (IO) has been used in MRI for more than 10 years (6). One of the most representative compounds is the monodisperse IO nanoparticle (MION) (7-9). MION has been used in MR contrast agent research because of its superparamagnetic IO core and is currently in clinical use. MION is coated with dextran to be biocompatible and is further stabilized via cross-linking with epichlorohydrin. This cross-linked IO (CLIO) can then be activated by reacting with ammonia, followed by conjugation with membrane translocation peptides.

An HIV-1 Tat peptide that consists of a core of 10 amino acids (amino acids 48-57) has been used to tag the nanoparticles CLIO-NH_2_. These nanoparticles are reported to be internalized into cells >100-fold more efficiently than non-modified magnetic particles (10). These CLIO-Tat agents have been used in in vitro and in vivo studies.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20AND%20tat%20AND%20synthesis)]

The synthesis of CLIO-Tat was described by Lewin et al. (11) and Dodd et al (12). CLIO-NH_2_ nanoparticles were prepared by coating CLIO nanoparticles with dextran, followed by cross-linking with epichlorohydrin and activation with ammonia (10, 13). Tat peptides were prepared using 9-fluorenylmethyloxycarbonyl (Fmoc) chemistry with incorporation of fluorescein isothiocyanate (FITC) during the peptide synthesis. Two Tat peptides were prepared: GGCGRKKRRQRRRK(FITC)-NH_2_ and GRKKRRQRRRGYK(FITC)C-NH_2_ (the italicized amino acids correspond to residues 48-57 of the Tat protein). These peptides were conjugated with CLIO-NH_2_ through either N-succinimidyl-3-(2-pyridyldithio)propionate (SPDP) (10, 11) or succinimidyl iodoacetate (SIA) (12, 14). The average number of peptides per CLIO nanoparticle ranges from 4.1 to 11.6 Tat/particle.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20AND%20tat%20AND%20%28in%20vitro%20or%20cell%29)]

CLIO-GGCGRKKRRQRRRK(FITC)-NH_2_ (average of 6.7 Tat peptides per CLIO crystal) was used to study the cell-labeling efficiency with murine lymphocytes, human natural killer cells, and HeLa cells (10). With murine lymphocytes, at a loading concentration of 100 μg of Fe/million cells in 1 ml media, there was an uptake of 2,535 ng of Fe/million cells corresponding to 12.7 × 10^6^ IO particles/cell. This was about 100-fold more efficient than CLIO-NH_2_ without Tat peptides attached. These internalized particles were located mostly in cytoplasm and nuclear compartments. A similar compound, CLIO-GRKKRRQRRRGYK(FITC)C-NH_2_ (CLIO-Tat), was used to study the effect on cellular uptake by changing the number of Tat peptides attached to the nanoparticle. The result showed that greater numbers of Tat peptides attached to the nanoparticles facilitated the cellular uptake in a nonlinear fashion (15).

In addition to its magnetic property, CLIO-Tat was tagged with diethylenetriamine pentaacetic acid (DPTA) so that it could be labeled with ^111^In to confirm the cellular uptake (11). Human hematopoietic CD34^+^ cells, mouse neural progenitor cells (C17.2), human CD4^+^ cells, and mouse splenocytes were used to quantitate cellular uptake. Similar labeling efficiencies were observed among these cell types. Up to 0.5-2 × 10^7^ nanoparticles/cell were internalized into the cells within 1 hour at 37 °C. Incorporation of the nanoparticles did not affect viability, differentiation, or proliferation of CD34^+^ cells. T cells loaded with CLIO-GRKKRRQRRRGYK(FITC)C-NH_2_ showed normal activation and activation-induced cell death (AICD), as well as normal upregulation of CD69, intercellular cell adhesion molecule-1 (ICAM-1) (CD54), L-selectin (CD62L), and Fas (12).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20AND%20tat%20AND%20rodentia)]

Cells loaded with radiolabeled CLIO-Tat were used to prove that the labeling of CLIO-Tat would not affect the in vivo distribution of labeled cells in mice. Human CD34^+^ cells were labeled with CLIO-Tat and ^111^In oxine or ^111^In oxine alone (as a control) and then injected into nonobese, severe combined immunodeficiency (NOD/SCID) mice (11). The biodistribution determined by ^111^In showed no difference between the control and the magnetically labeled cells. Approximately 4% injected dose (ID)/g tissue of cells migrated to bone marrow, 15% ID/g tissue were found in spleen, and 22% ID/g tissue in liver. MRI was performed on the bone marrow of NOD/SCID mice 24 h after the injection. The injected human CD34^+^ cells were detectable at single-cell level and could be recovered by magnetic separation columns.

CLIO-Tat was used to track immune cells in autoimmune diseases (16). Freshly isolated lymphocytes from NOD mice were labeled with CLIO-Tat and then injected into NOD/SCID mice. MRI showed that these CLIO-Tat–labeled cells infiltrated the pancreatic islets of NOD/SCID mice.

T cells isolated from B6 mice were loaded with CLIO-Tat and injected back into the B6 mice through the tail vein (12). There was a 20% reduction of MRI signal intensity in the spleen at 3 h after the injection, which indicated homing of CLIO-Tat–loaded T cells. The intensity remained low even after 24 h.

With 9.7 Tat peptides (GRKKRRQRRRGYK(FITC)C-NH_2_) attached to the CLIO-NH_2_ nanoparticles, the blood half-life was reduced to 47 ± 6 min compared to 655 ± 37 min for the unmodified CLIO-NH_2_ (14). The shortened blood half-life of CLIO-Tat is likely caused by the enhanced interaction of CLIO-Tat with phagocytes mediated either by the Tat peptide itself or by enhanced opsonin-mediated phagocytosis. At an injection concentration of 10 mg Fe/kg, CLIO-NH_2_ and CLIO-Tat showed similar biodistributions in female Balb C mice. The highest concentration appeared in the liver, spleen, and lymph nodes, ranging from 8.80 to 6.11% ID/g tissue. Results from fluorescence microscopy of the mouse liver showed that CLIO-NH_2_ was concentrated in endothelial and Kupffer cells surrounding hepatic blood vessels. However, CLIO-Tat presented as numerous discrete foci throughout the parenchyma 24 h after the intravenous injection. This indicated that CLIO-Tat somehow passed from the vascular compartment and through cells surrounding vessels to achieve the parenchymal distribution. The fluorescence distributed in the liver cells appeared to be similar to that of HeLa cells, where CLIO-Tat showed pronounced nuclear accumulation. It was suggested that, while the nanoparticles determine the organ biodistribution, Tat peptide conjugation to the nanoparticles broadens the intrahepatic distribution to the parenchyma and also significantly reduces the blood half-life.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20AND%20tat%20AND%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No relevant publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20AND%20tat%20AND%20%28primate%20not%20human%29)]

No relevant publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CLIO%20AND%20tat%20AND%20human)]

No relevant publication is currently available.

## References

1 Derossi D, Calvet S, Trembleau A, Brunissen A, Chassaing G, Prochiantz A. (1996). Cell internalization of the third helix of the Antennapedia homeodomain is receptor-independent. J Biol Chem.
2 Elliott G, O'Hare P. (1997). Intercellular trafficking and protein delivery by a herpesvirus structural protein. Cell.
3 Phelan A, Elliott G, O'Hare P. (1998). Intercellular delivery of functional p53 by the herpesvirus protein VP22. Nat Biotechnol.
4 Avrameas A, Ternynck T, Nato F, Buttin G, Avrameas S. (1998). Polyreactive anti-DNA monoclonal antibodies and a derived peptide as vectors for the intracytoplasmic and intranuclear translocation of macromolecules. Proc Natl Acad Sci U S A.
5 Fawell S, Seery J, Daikh Y, Moore C, Chen LL, Pepinsky B, Barsoum J. (1994). Tat-mediated delivery of heterologous proteins into cells. Proc Natl Acad Sci U S A.
6 6. P, Cosgrove DO, Grainger RG, eds. Textbook of Contrast Media. 1st ed. 1999, Isis Medical Media Ltd.: . 612.
7 Schoepf U, Marecos EM, Melder RJ, Jain RK, Weissleder R. (1998). Intracellular magnetic labeling of lymphocytes for in vivo trafficking studies. Biotechniques.
8 Yeh TC, Zhang W, Ildstad ST, Ho C. (1993). Intracellular labeling of T-cells with superparamagnetic contrast agents. Magn Reson Med.
9 Yeh TC, Zhang W, Ildstad ST, Ho C. (1995). In vivo dynamic MRI tracking of rat T-cells labeled with superparamagnetic iron-oxide particles. Magn Reson Med.
10 Josephson L, Tung CH, Moore A, Weissleder R. (1999). High-efficiency intracellular magnetic labeling with novel superparamagnetic-Tat peptide conjugates. Bioconjug Chem.
11 Lewin M, Carlesso N, Tung CH, Tang XW, Cory D, Scadden DT, Weissleder R. (2000). Tat peptide-derivatized magnetic nanoparticles allow in vivo tracking and recovery of progenitor cells. Nat Biotechnol.
12 Dodd CH, Hsu HC, Chu WJ, Yang P, Zhang HG, Mountz JD, Zinn K, Forder J, Josephson L, Weissleder R, Mountz JM, Mountz JD. (2001). Normal T-cell response and in vivo magnetic resonance imaging of T cells loaded with HIV transactivator-peptide-derived superparamagnetic nanoparticles. J Immunol Methods.
13 Hogemann D, Josephson L, Weissleder R, Basilion JP. (2000). Improvement of MRI probes to allow efficient detection of gene expression. Bioconjug Chem.
14 Wunderbaldinger P, Josephson L, Weissleder R. (2002). Tat peptide directs enhanced clearance and hepatic permeability of magnetic nanoparticles. Bioconjug Chem.
15 Zhao M, Kircher MF, Josephson L, Weissleder R. (2002). Differential conjugation of tat peptide to superparamagnetic nanoparticles and its effect on cellular uptake. Bioconjug Chem.
16 Moore A, Sun PZ, Cory D, Hogemann D, Weissleder R, Lipes MA. (2002). MRI of insulitis in autoimmune diabetes. Magn Reson Med.